# BBQ650-Pro-Leu-Gly-Val-Arg-Lys(Cy5.5)-Glu-Lys(^64^Cu-DOTA)-OH

Chemical name: | BBQ650-Pro-Leu-Gly-Val-Arg-Lys(Cy5.5)-Glu-Lys(^64^Cu-DOTA)-OH
Abbreviated name: | BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Multimodality: positron emission tomography (PET), optical, near-infrared fluorescence (NIRF) imaging
Source of signal/contrast: | ^64^Cu, Cy5.5
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for the permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). The peptide Pro-Leu-Gly-Val-Arg-NH_2_ (PLGVR) was found to be a MMP substrate and is cleaved between the Gly (G) and Val (V) residues (9). Huang et al. (10) linked a fluorescence quencher BBQ650 to the N-terminus of Pro-Leu-Gly-Val-Arg-Lys-Glu-Lys (PLGVRKEK), a Cy5.5 molecule to the Lys closer to BBQ650, and a DOTA molecule to the ɣ-amino group of the C-terminus Lys (K) residue to form BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH for optical imaging of protease activity in vivo. Upon MMP cleavage, VR-K(Cy5.5)-E-K(DOTA)-OH is released with a greater fluorescence signal and accumulated at the sites of protease activity. For positron emission tomography (PET) imaging, the agent was labeled with ^64^Cu to form BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH. BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH accumulated in human U87MG glioblastoma xenografts as determined with optical imaging in nude mice.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP9 (http://www.ncbi.nlm.nih.gov/gene/4318), MMP13 (http://www.ncbi.nlm.nih.gov/gene/4322))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://omim.org/entry/120360), MMP9 (http://omim.org/entry/120361), MMP13 (http://omim.org/entry/600108))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR)]

BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH was prepared with solid-phase peptide synthesis (10). BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH exhibited >98% purity as determined with high-performance liquid chromatography (HPLC) . The identity of BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH was confirmed with HPLC and electroscopy ionization mass spectra. BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH was incubated with ^64^CuCl_2_ in 0.1 M sodium acetate buffer (pH 5.5) for 60 min at 40°C. BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH was purified with HPLC, with >95% radiochemical yield and >98% radiochemical purity. The specific activity was 4.2 MBq/nmol (0.11 mCi/nmol). BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH was >97% and >80% intact in phosphate-buffered saline (pH 7.4) and mouse serum, respectively, after 24 h of incubation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR%20and%20in%20vitro)]

Huang et al. (10) showed that BBQ650-PLGVR-K(Cy5.5)-E-K(DOTA)-OH was cleaved with purified MMP13 enzyme into two fragments, BBQ650-PLG and VR-K(Cy5.5)-E-K(DOTA)-OH, as measured with HPLC. There was a time-dependent increase in fluorescence signal, with 7.2-fold increased at 120 min of incubation. The cleavage of the probe and the increase in fluorescence signal were inhibited by a broad-spectrum MMP inhibitor III.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR%20and%20rodentia)]

Huang et al. (10) performed in vivo optical imaging studies in nude mice (n = 3/group) bearing U87MG xenografts for 120 min after intratumor injection of BBQ650-PLGVR-K(Cy5.5)-E-K(^64^Cu-DOTA)-OH (2 nmol). Fluorescence signal was observed within 5 min of injection and gradually increased with time. The signal intensity was 6 × 10^8^ p/s/cm^2^/sr at 5 min and 13 × 10^8^ p/s/cm^2^/sr at 120 min. Injection of the broad-spectrum MMP inhibitor III 30 min before the probe inhibited the signal intensity nearly to the background level at 5–120 min. In vivo PET imaging scans were not performed in these tumor-bearing mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLGVR%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Bae M., Cho S., Song J., Lee G.Y., Kim K., Yang J., Cho K., Kim S.Y., Byun Y. (2003). Metalloprotease-specific poly(ethylene glycol) methyl ether-peptide-doxorubicin conjugate for targeting anticancer drug delivery based on angiogenesis. Drugs Exp Clin Res.
10 Huang C.W., Li Z., Conti P.S. (2012). Radioactive smart probe for potential corrected matrix metalloproteinase imaging. Bioconjug Chem.